# ^99m^Tc-(RR,SS)-4,8-diaza-3,6,6,9-tetramethylundecane-2,10-dione bisoxime

Chemical name: | ^99m^Tc-(RR,SS)-4,8-diaza-3,6,6,9-tetramethylundecane-2,10-dione bisoxime
Abbreviated name: | ^99m^Tc-HMPAO
Synonym: | Ceretec™ Technetium-exametazime; Technetium-99-HMPAO; Technetium-99m-HMPAO; Technetium-99mTc-HMPAO; (99M)Tc-hexamethylpropyleneamine oxime; 99mTc-(RR,SS)-4,8-diaza-3,6,6,9-tetramethylundecane-2,10-dione bisoxime (SP-5-15)-((Rel-(3R,3'R)-3,3'-((2,2-dimethyl-1,3-propanediyl)di(imino-kappaN))bis(2-butanone)di(oximato-kappaN)) (3-))oxotechnetium-99Tc; [2,2-dimethyl-3-[(3E)-3-oxidoiminobutan-2-yl]azanidyl-propyl]-[(3E)-3-hydroxyiminobutan-2-yl]azanide; oxotechnetium
Agent Category: | Compound
Target: | Intra-cellular components
Target Category: | Binding
Method of detection: | Single photon emissiom computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO)]

Timely diagnosis of cerebrovascular diseases (CVD) including stroke, transient ischemic attack, reversible ischemic neurological deficit and multi-infaract dementia etc. is important for the appropriate treatment of patients. Cerebral blood flow (CBF) imaging is a routine technique used for the diagnosis of CVD. Technetium (^99m^Tc) labeled d,l-hexamethyl propylene-amineoxime (^99m^Tc-HMPAO) is widely used as a noninvasive cerebral perfusion imaging agent for the diagnosis of CVD (1). ^99m^Tc-HMPAO is able to cross the blood brain barrier, is highly lipophillic and easily diffuses across the cell membrane. In the cell it is believed to be rapidly hydrolyzed into more polar hydrophilic species that are retained within the cells and can be used for imaging of the brain (1). In addition, ^99m^Tc-HMPAO has also been used to label leukocytes for the detection of inflammation and infections (2, 3) and bone marrow mononuclear cells to track them under in vivo conditions (4).

The synthesis and use of ^99m^Tc-HMPAO is patented in the US (5) and is available commercially as a kit for intravenous use (6). The kit is approved (http://md.gehealthcare.com/ceretec) by the United States Food and Drug Administration for the detection of altered regional cerebral perfusion in stroke or for leukocyte labeled scintigraphy as an adjunct for the localization of intra-abdominal infection and inflammatory bowel disease (IBD).

.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO%20synthesis)]

The synthesis of ^99m^Tc-HMPAO has been described in a US patent (5). To start, 2,3-butanedione monoxime was dissolved in benzene containing acetic acid and the solution was refluxed in a nitrogen atmosphere. A solution of 2,2-dimethyl-1,3-propanediamine in benzene was added and the solution refluxed for another 16 h under nitrogen. The solution was then allowed to cool to room temperature. The resulting solid was filtered under suction and washed with cold (-40^o^C) acetonitrile to obtain a fine white powder. The powder was dried under high vacuum for 2 h to obtain 4,8-diaza-3,6,6,9-tetramethyl-3,8-undecadiene-2,10-dione bisoxime, a diimine, with a 60% yield.

The diimine was slurried in 95% aqueous ethanol at 0^o^C and sodium borohydrate was added to it over half an hour. The mixture was stirred at 0^o^C for 2 h followed by addition of water stirring for another 2 h. The ethanol was removed under vacuum and more water was added to the mixture. The pH of the solution was adjusted to 11 to obtain a white solid that was filtered, washed with some water, and dried under vacuo to obtain crude HMPAO. Double crystallization from acetonitrile gave the pure product with a yield of 80%.

Labeling of HMPAO should be done carefully, with adherence to all precautions, as described in the product insert (http://md.gehealthcare.com/shared/pdfs/pi/ceretec.pdf) by the kit manufacturer (6). The use of methylene blue is recommended by the manufacturer to stabilize ^99m^Tc-HMPAO only for cerebral scintigraphy with a dose range of 10-20 mCi (370-740 MBq). According to the manufacturer methylene blue should not be used to stabilize ^99m^Tc-HMPAO for the labeling of leukocytes, as described in the product insert (6). To visualize intra-abdominal infection or inflammation, the recommended dose for a normal adult (70 kg) is 7-25 mCi (0.259-0.925 GBq), as labeled leukocytes.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO%20in%20vitro)]

A study was performed to compare the in vitro labeling efficiency (LE) and cell viability of autologous leukocytes labeled with ^99m^Tc-stannous (^99m^Tc-SnF_2_) colloid kit and ^99m^Tc-HMPAO (7). The cells were then used to study IBD. During the study the quantity and quality of spontaneously released ^99m^Tc (SR) from labeled cells at several time points after labeling was also evaluated. Both radiopharmaceuticals were non-toxic to the leukocytes. Labeling with ^99m^Tc-SnF_2_ was observed to give a higher LE than with ^99m^Tc-HMPAO; however, a higher amount of radiolabeled colloids, compared to the radioactivity from ^99m^Tc-HMPAO labeled cells, was released from the cells over a 4 h period. It was concluded while ^99m^Tc-HMPAO is physiological excreted into the gastrointestinal tract, ^99m^Tc-SnF_2_ can be re-takenup in vivo by the reticulo-endothelial cells of the liver and spleen. These findings suggest that ^99m^Tc-SnF_2_ leukocytes may be better than ^99m^Tc-HMPAO leukocytes to study IBD.

The contribution of different cell types on ^99m^Tc-HMPAO retention in the brain was investigated in vitro using primary cultures of mouse cortical astrocytes and neurons (8). The data indicated that astrocytes may constitute a prominent site of ^99m^Tc-HMPAO retention and most likely contributed significantly to the SPECT signal. Data from the study also suggested that specific alterations in glial cell metabolism under some diseased states could explain the flow-independent changes in ^99m^Tc-HMPAO retention in the brain, as observed by scintigraphy.

## Animal Studies

### Rodents

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO%20rodentia)]

Using a scintigraphic method the in vivo distribution of naïve and memory CD8+ lymphocytes labeled with ^99m^Tc-HMPAO was studied in syngenic rats (9). The memory cells were shown to recirculate into the liver and lungs. In the same study total blood lymphocytes were shown to accumulate at the sites of inflammation in inflamed animals.

The possible use of ^99m^Tc-HMPAO biodistribution to determine the glutathione (GSH) status of tumors in a mouse model has been investigated (10). From this study it was concluded that ^99m^Tc-HMPAO may be useful to estimate the GSH status of various tumors and this indicator can be used for the development of an appropriate anticancer therapy.

A study was performed to evaluate the use of ^99m^Tc-HMPAO scintigraphy to assess neutrophil trafficking in a mouse model of dextran sulfate sodium (DSS)-induced colitis (11). The uptake of ^99m^Tc-HMPAO labeled neutrophils was determined with dedicated animal pinhole SPECT in the DSS-induced colitis animals. It correlated well with the histologic observations (R = 0.81) and the wet colon weight (R = 0.87) and moderately with clinical weight loss (R = 0.62). When neutrophil migration was blocked with a CD97 antibody a significant reduction in the neutrophil uptake ratio (P < 0.01) was observed. It was concluded this technique could be used to study inflammation and neutrophil recruitment in an in vivo experimental colitis model.

Spermatozoa labeled with ^99m^Tc-HMPAO were inseminated into female rabbits and dynamic scintigraphic studies were performed on the animals up to 12 hr after the procedure (12). The labeled spermatozoa had a similar in vivo behavior as the native spermatozoa. The absolute spermatozoa numbers could be determined noninvasively, and reliably, within the different parts of the female genital tract at various time points after insemination. According to the investigators ^99m^Tc-HMPAO can be used to noninvasively follow the dynamic distribution of spermatozoa in the female genital tract.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO%20Other%20Non-Primate%20Mammals)]

^99m^Tc-HMPAO radiolabeled leukocytes and scintigraphy were utilized to assess the inflamed feline pancreas (13). The radiolabeled leukocytes were used to visualize pancreatic inflammation that was best visualized at 4 h after administration of the cells. The appearance and contrast enhancement pattern of the inflamed pancreas was observed to be different from normal and scintigraphy allowed a better visualization of the pancreas.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-HMPAO%20Non-Human%20Primates)]

A baboon (Papio ursinus) model was used for the in vivo determination of CBF, with a split-dose ^99m^Tc-HMPAO single photon emission computed tomography (SPECT) method (14). The study showed that the CBF non-human primate model was useful to investigate vasoactive drugs that act through different pharmacological modes.

Using ^99m^Tc-HMPAO scintigraphy on baboons (P ursinus) it was shown a combined treatment of the normal animals with zolpidem and flumazenil, that target the omega receptors of the gamma-aminobutyric acid receptor system, decreased the brain blood flow of the animals (15). Based on these results an involvement of the omega receptors in the brain blood flow of the animals was suggested by Clauss et. al. (15). They hypothesized that an up- or down-regulation of these receptors could contribute to the observed responses in the baboons that are similar to those observed in brain injured patients.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20HMPAO%20human)]

Clinical trials to compare ^99m^Tc-HMPAO labeled leukocytes with those labeled with radioactive indium (^111^In) have been described by the manufacturer in the product kit insert (6). Based on these studies visualization after 2 to 4 h showed the ^99m^Tc-HMPAO labeled leukocytes had a 95-100% sensitivity and 62-85% specificity for the detection of intra-abdominal infection or inflammation. According to the manufacturer, images obtained after 24 h give inconsistent information and cautions that images obtained with either ^99m^Tc or ^111^In labeled leukocytes at this time point should be evaluated carefully for interpretation.

The use of a hybrid SPECT/computed tomography technique with ^99m^Tc-HMPAO labeled leukocytes to detect bone and joint infections was described by Filippi and Schillaci (16). The hybrid technique was shown to improve imaging with ^99m^Tc-HMPAO labeled leukocytes and provide an accurate anatomic localization and precise definition of the infection. In another study the prognostic utility of ^99m^Tc-HMPAO labeled leukocytes in IBD was evaluated (17). In this study it was shown leukocyte scintigraphy may have a prognostic value for the management of IBD.

Uslu et. al. demonstrated ^99m^Tc-HMPAO labeled leukocytes could be used accurately and rapidly for the evaluation of acute pancreatitis in patients (2). Scintigraphy has also been used to track ^99m^Tc-HMPAO labeled bone marrow mononuclear cells in a cardiovascular stem cell study in a man (4).

Using ^99m^Tc-HMPAO scintigraphy Nishimura et. al. (18) showed that a decreased blood flow in the frontal lobe of Alzheimer’s disease (AD) patients correlated with the reduced cognitive functions observed in these individuals. They also showed this technique could be used to follow AD progression in the patients. ^99m^Tc-HMPAO scintigraphy was shown to be useful for the presurgical evaluation of patients with refractory seizures observed during epilepsy (19). Kemp et. al. reported ^99m^Tc-HMPAO scintigraphy was of limited value to diagnose of Lewis body dementia (20). An altered regional CBF was demonstrated by ^99m^Tc-HMPAO scintigraphy in patients with primary hyperparathyroidism (21). It was shown scintigraphy could be used to determine the degree of regional CBF abnormalities in such patients.

## Supplemental Information

[Disclaimer]

## References

1 Ding H.J., Huang Y.F., Tzeng C.C., Wei L.M., Yeh S.J. (1999). Synthesis of Tc-D,D-HMPAO and Tc-L,L-HMPAO and their comparison of chemical and biological properties. Bioorg Med Chem Lett.
2 Uslu H., Varoglu E., Balik A., Yildirim M., Bayrakdar R., Seven B. (2007). Scintigraphic evaluation of acute pancreatitis patients with 99mTc-HMPAO-labelled leukocytes. Nucl Med Commun.
3 Roca M., Martin-Comin J., Becker W., Bernardo-Filho M., Gutfilen B., Moisan A., Peters M., Prats E., Rodrigues M., Sampson C., Signore A., Sinzinger H., Thakur M. (1998). A consensus protocol for white blood cells labelling with technetium-99m hexamethylpropylene amine oxime. International Society of Radiolabeled Blood Elements (ISORBE). Eur J Nucl Med.
4 Mesquita C.T., Correa P.L., Felix R.C., Azevedo J.C., Alves S., Oliveira C.C., Sousa A.L., Borojevic R., Dohmann H.F. (2005). Autologous bone marrow mononuclear cells labeled with Tc-99m hexamethylpropylene amine oxime scintigraphy after intracoronary stem cell therapy in acute myocardial infarction. J Nucl Cardiol.
5 Cunning, L.R., D.P. Nowotnik, R.D. Neirinckx, and I.M. Piper, Complexes of technetiun-99m with propyl amine oximes, U.S. Patent, Editor. 1988, Amersham International, plc.
6 GE, H., Ceretec TM Kit for the preparation of technetium Tc99m Exametazime injection. 2006, GE Healthcare.
7 Capriotti G., D'Alessandria C., Garin E., Weber E., Devillers A., Lehmann K., Corsetti F., Lecloirec J., Meller J., Becker W., Moisan A., Signore A. (2004). An in vitro study to compare 99mTc-stannous colloids and 99mTc-HMPAO for labelling human leukocytes. Q J Nucl Med Mol Imaging.
8 Zerarka S., Pellerin L., Slosman D., Magistretti P.J. (2001). Astrocytes as a predominant cellular site of (99m)Tc-HMPAO retention. J Cereb Blood Flow Metab.
9 Fulgenzi A., Casati R., Colombo F.R., Gasparini M., Ferrero E., Bondanza A., Gerundini P., Ferrero M.E. (2004). Distribution of 99mTc-labeled lymphocytes in control and inflamed rats. Nucl Med Biol.
10 Shimura N., Musya A., Hashimoto T., Kojima S., Kubodera A., Sasaki T. (2000). Usefulness of (99m)Tc-d,l-HMPAO for estimation of GSH content in tumor tissues. Nucl Med Biol.
11 Bennink R.J., Hamann J., de Bruin K., ten Kate F.J., van Deventer S.J., te Velde A.A. (2005). Dedicated pinhole SPECT of intestinal neutrophil recruitment in a mouse model of dextran sulfate sodium-induced colitis. J Nucl Med.
12 Bockisch A. (1993). Sperm cell dynamics in the female rabbit genital tract after insemination monitored by radiolabeled spermatozoa. J Nucl Med.
13 Head L.L., Daniel G.B., Becker T.J., Lidbetter D.A. (2005). Use of computed tomography and radiolabeled leukocytes in a cat with pancreatitis. Vet Radiol Ultrasound.
14 Oliver D.W., Dormehl I.C., Louw W.K. (2005). Non-human primate SPECT model for determining cerebral perfusion effects of cerebrovasoactive drugs acting via multiple modes of pharmacological action. J Neurol Sci.
15 Clauss R.P., Dormehl I.C., Kilian E., Louw W.K., Nel W.H., Oliver D.W. (2002). Cerebral blood perfusion after treatment with zolpidem and flumazenil in the baboon. Arzneimittelforschung.
16 Filippi L., Schillaci O. (2006). Usefulness of hybrid SPECT/CT in 99mTc-HMPAO-labeled leukocyte scintigraphy for bone and joint infections. J Nucl Med.
17 Carrera D., Domenech A., Mora J., Ballester R., Roca M., Jimenez R.I., Verdura B., Baliellas C., Guardiola J., Martin-Comin J. (2006). , and , . ,.
18 Nishimura T., Hashikawa K., Fukuyama H., Kubota T., Kitamura S., Matsuda H., Hanyu H., Nabatame H., Oku N., Tanabe H., Kuwabara Y., Jinnouchi S., Kubol A. (2007). Decreased cerebral blood flow and prognosis of Alzheimer's disease: a multicenter HMPAO-SPECT study. Ann Nucl Med.
19 Van Paesschen W. (2004). Ictal SPECT. Epilepsia.
20 Kemp P.M., Hoffmann S.A., Tossici-Bolt L., Fleming J.S., Holmes C. (2007). Limitations of the HMPAO SPECT appearances of occipital lobe perfusion in the differential diagnosis of dementia with Lewy bodies. Nucl Med Commun.
21 Cermik T.F., Kaya M., Ugur-Altun B., Bedel D., Berkarda S., Yigitbasi O.N. (2007). Regional cerebral blood flow abnormalities in patients with primary hyperparathyroidism. Neuroradiology.